# (2S,3S)-(2-[^11^C]Methoxy-5-tetrazol-1-ylbenzyl)(2-phenylpiperidin-3-yl)amine

Chemical name: | (2S,3S)-(2-[^11^C]Methoxy-5-tetrazol-1-ylbenzyl)(2-phenylpiperidin-3-yl)amine
Abbreviated name: | [^11^C]GR203040
Synonym:
Agent Category: | Compound
Target: | NK_1_ receptor
Target Category: | Receptor binding
Method of detection: | Positron Emission Tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=GR203040)]

(2S,3S)-(2-[^11^C]Methoxy-5-tetrazol-1-ylbenzyl)(2-phenylpiperidin-3-yl)amine ([^11^C]GR203040) is a radioligand developed for positron emission tomography (PET) imaging of neurokinin 1 (NK_1_) receptors [substance P (SP) receptors] in the central nervous system (CNS) (1).

Tachykinins are peptides comprising 10−12 amino acids that share a common carboxy-terminal sequence “Phe-X-Gly-Leu-Met-amide” where “X” may vary but is always a hydrophobic residue that is either aromatic or β-branched aliphatic (2-4). This peptide family consists of SP, neurokinin A (NK_A_), and neurokinin B (NK_B_). The tachykinin peptides mediate their effects by specific G protein−coupled receptors. These receptors are divided into three subtypes: NK_1_, (formerly the SP receptor), NK_2_ (formerly the substance K/substance E receptor/NK_A_ receptor), and NK_3_ (formerly the NK_B_ receptor). The effects of SP are mediated primarily via the NK_1_ receptor subtypes. There is evidence that SP behaves like a neurotransmitter involved in regulation of emotional and behavioral responses to a range of noxious and stressful stimuli (5). SP may also play a role in neurogenic inflammation, vasomotor control, and many gastrointestinal functions. Studies in the brain have shown that SP is found in the neocortex, limbic areas, habenula, periaqueductal gray matter, midbrain nuclei, and is especially enriched in the basal ganglia. There is little SP in the cerebellum. The distribution of the NK_1_ receptors in the brain generally corresponds to that of SP.

SP-NK_1_ receptor pathways are found in both the CNS and the peripheral nervous system. The CNS pathways have been implicated in the pathophysiology of pain, nausea/emesis, and depression disorders (6). PET and single-photon emission computed tomography of radioligands targeting NK_1_ receptors can visualize and allow the study of CNS NK_1_ receptors in normal and pathologic states. These studies can identify the degree of receptor occupancy in patients with depression and the change in response to therapy (6). A number of NK_1_ selective agonists and antagonists have been successfully labeled, but they failed to provide a specific signal in vivo (6, 7). Ward et al. (8) reported the antiemetic, pharmacokinetic, and metabolic profile of the potent NK_1_ receptor antagonist CP-99,994. They also reported that a tetrazolyl-substituted analog, GR203040, had high metabolic stability, low lipophilicity, and high NK_1_ receptor affinity. ^11^C-labeled GR205171 and its trifluoromethyl analog, [^11^C]GR205171, were studied to be used as a PET ligand to characterize NK_1_ receptor binding (1).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=GR203040%20AND%20synthesis)]

Ward et al. (8) reported the synthesis of GR203040, a tetrazolyl-substituted analogue of CP-99,994. Bergstrom et al. (1) investigated two approaches for the radiosynthesis of [^11^C]GR203040. One approach used an N-di-BOC protected GR203040, and another approach used a non-protected GR203040. They reported that the non-protected precursor approach had the shorter synthesis time and higher radiochemical yields. In this method, GR203040 was dissolved in dichloromethane and mixed with tetrabutylammonium hydroxide. The mixture was heated and shaken for 2 min. The solvent was then evaporated and the residue was redissolved in N,N-dimethylformamide. [^11^C]methyl iodide was trapped in this solution at room temperature. The mixture was then heated at 80ºC for 5 min. [^11^C]GR203040 was obtained and purified by high-performance liquid chromatography. The radiochemical yield was 45% based on [^11^C]methyl iodide with a total synthesis time of 45 min. The radiochemical purity was >98%, and the specific activity was 20−120 GBq/ μmol. (0.54−3.24 Ci/μmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=GR203040%20AND%20in%20vitro)]

Beattie et al. (9) studied the in vitro NK_1_ receptor binding affinity of GR203040 in stably transfected Chinese hamster ovary (CHO) cells and U373 MG astrocytoma cells (human receptors), as well as cerebral cortical membranes from rat, ferret, and gerbil cortex. Based on inhibition of ^3^H-labeled SP binding, the inhibition constant (pK_i_) values were calculated to be 10.3 ± 0.1 (human recombinant receptors in CHO cells), 10.5 ± 0.2 (U373 MG cells), 8.6 (rat cortex), 10.1 (gerbil cortex), and 10.1 (ferret cortex). In comparison, the pK_i_ values of CP-99,994 and GR205171 for the human NK_1_ receptors in CHO cells were 9.6 ± 0.1 (n = 20) and 10.6 ± 0.22 (n = 4−5), respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=GR203040%20AND%20rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=GR203040%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=GR203040%20AND%20%28primate%20NOT%20human%29)]

Bergstrom et al. (1) conducted PET imaging of [^11^C]GR203040 in rhesus monkeys. The monkeys were given either a low i.v. dose [30 MBq (0.81 mCi)] or a high i.v. dose [150 MBq (4.1 mCi)] of [^11^C]GR203040. After injection, a constant plasma level of a standard uptake value (SUV) of 1.0 was reached within 10 min. There was a significant and rapid uptake in the brain. The brain radioactivity level reached a plateau with no washout during the examination time of 50 min. The thalamus had the highest level of radioactivity. The radioactivity levels of all brain structures increased slightly with time. The SUV of the thalamus was 1.5. The SUVs of other brain structures were approximately 1.1. Pre-treatment with unlabeled GR203040 decreased the radioactivity level by 20%. In comparison, [^11^C]GR205171 had a SUV of 2.8 at 50 min in the striatum. The authors concluded that [^11^C]GR203040 had less favorable properties than [^11^C]GR205171 for the in vivo characterization of NK_1_ receptors. Based on the fact that GR205171 is slightly more lipophilic and had higher brain uptake at all doses, the authors suggested that GR205171 had a better penetration of the blood-brain barrier.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=GR203040%20AND%20human)]

No publication is currently available.

## References

1 Bergstrom M., Fasth K.J., Kilpatrick G., Ward P., Cable K.M., Wipperman M.D., Sutherland D.R., Langstrom B. (2000). Brain uptake and receptor binding of two [11C]labelled selective high affinity NK1-antagonists, GR203040 and GR205171--PET studies in rhesus monkey. Neuropharmacology.
2 Hietala J., Nyman M.J., Eskola O., Laakso A., Gronroos T., Oikonen V., Bergman J., Haaparanta M., Forsback S., Marjamaki P., Lehikoinen P., Goldberg M., Burns D., Hamill T., Eng W.S., Coimbra A., Hargreaves R., Solin O. (2005). Visualization and quantification of neurokinin-1 (NK1) receptors in the human brain. Mol Imaging Biol.
3 Severini C., Improta G., Falconieri-Erspamer G., Salvadori S., Erspamer V. (2002). The tachykinin peptide family. Pharmacol Rev.
4 Datar P., Srivastava S., Coutinho E., Govil G. (2004). Substance P: structure, function, and therapeutics. Curr Top Med Chem.
5 Mantyh P.W. (2002). Neurobiology of substance P and the NK1 receptor. J Clin Psychiatry.
6 Hargreaves R. (2002). Imaging substance P receptors (NK1) in the living human brain using positron emission tomography. J Clin Psychiatry.
7 Solin O., Eskola O., Hamill T.G., Bergman J., Lehikoinen P., Gronroos T., Forsback S., Haaparanta M., Viljanen T., Ryan C., Gibson R., Kieczykowski G., Hietala J., Hargreaves R., Burns H.D. (2004). Synthesis and characterization of a potent, selective, radiolabeled substance-P antagonist for NK1 receptor quantitation: ([18F]SPA-RQ). Mol Imaging Biol.
8 Ward P., Armour D.R., Bays D.E., Evans B., Giblin G.M., Heron N., Hubbard T., Liang K., Middlemiss D., Mordaunt J., Naylor A., Pegg N., Vinader M.V., Watson S.P., Bountra C., Evans D.C. (1995). Discovery of an orally bioavailable NK1 receptor antagonist, (2S,3S)-(2-methoxy-5-tetrazol-1-ylbenzyl)(2-phenylpiperidin-3-yl)amine (GR203040), with potent antiemetic activity. J Med Chem.
9 Beattie D.T., Beresford I.J., Connor H.E., Marshall F.H., Hawcock A.B., Hagan R.M., Bowers J., Birch P.J., Ward P. (1995). The pharmacology of GR203040, a novel, potent and selective non-peptide tachykinin NK1 receptor antagonist. Br J Pharmacol.